# ^125^I Labeled-mesenchymal-epithelial transition factor binding peptide

Chemical name: | ^125^ILabeled-mesenchymal-epithelial transition factor binding peptide | [image]
Abbreviated name: | [^125^I]cMBP | [image]
Synonym: | | [image]
Agent Category: | Ligand | [image]
Target: | Mesenchymal-epithelial transition factor receptor (c-Met); hepatocyte growth factor receptor (HGFR) | [image]
Target Category: | Receptor | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^125^I | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of cMBP.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5)]

The hepatocyte growth factor (HGF) is the only known ligand of the mesenchymal-epithelial transition factor (c-Met) (also known as the HGF receptor) that has an important function, including cell development, proliferation, scattering, migration, and angiogenesis, all of which are necessary for the survival and repair of tissues (1). c-Met is known to mediate its activity through an intracellular tyrosine kinase (TK) that activates different signal transduction pathways, leading to initiation of the various cell processes (2). Also, deregulation of c-Met activity due to paracrine/autocrine activation, overexpression, or a mutation promotes the development of a neoplastic cell phenotype (2). Overexpression of c-Met and HGF has been associated with a poor prognosis and survival of the patient (3), suggesting that the c-Met receptor may be a suitable target for the detection of cancers at an early stage, which could help in the development of an appropriate treatment regimen to improve patient prognosis (4). c-Met is the target of several drugs under evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=HGFR) approved by the United States Food and Drug Administration. Investigators recently generated a monoclonal antibody (mAb) that inhibits the HGF–c-Met interaction and identified the active mAb against a surface epitope peptide as KSLSRHDHIHHH, which was designated as the c-Met binding peptide (cMBP) (5). The cMBP and its derivatives (containing a linker that was either a tri-amino acid linker, Gly-Gly-Gly (GGG), or an aliphatic carbon, 8-aminooctanoic acid (AOC)) were labeled with ^125^I to generate ^125^I-cMBP, 1^25^I-cMBP-GGG, and ^125^I-cMBP-AOC, and these agents were used to detect c-Met TK-positive tumor xenografts in mice (6). From this study the investigators concluded that although ^125^I-cMBP was suitable for the imaging of c-Met TK-expressing tumors, the signal to background obtained from this nuclide was not very high, and the results could probably be improved by using another radionuclide and/or by modifying the linkers.

In an attempt to generate a c-Met–positive tumor imaging agent superior to ^125^I-cMBP, ^125^I-cMBP-GGG, and ^125^I-cMBP-AOC, investigators conjugated a near-infrared (NIR) fluorescent dye, cyanine 5.5 (Cy5.5), to cMBP-GGG and cMBP-AOC to obtain cMBP-GGG-Cy5.5 and cMBP-AOC-Cy5.5 (4). The Cy5.5-conjugated cMBP derivatives were then evaluated for the NIR imaging of c-Met–positive xenograft tumors in a mouse model.

This chapter describes the in vitro and in vivo characterization of only ^125^I-cMBP. The other c-Met imaging agents (1^25^I-cMBP-GGG, ^125^I-cMBP-AOC, cMBP-GGG-Cy5.5, and cMBP-AOC-Cy5.5) are described in separate MICAD chapters (7-10).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20synthesis)]

The synthesis of cMBP was described previously (4). Briefly, the cMBP peptide was synthesized using Fmoc chemistry, with a purity of 90%. The ^125^I labeling of cMBP was done by the chloramine T method, and the reaction was terminated with sodium bisulfite. The radiochemical purity of the labeled compound was reported to be between 90% and 95% at 24 h after the labeling as determined with instant thin-layer chromatography (ITLC). The stability of ^125^I-cMBP in human serum was reported to be 90% at 1 h and 88% at 4 h as determined with ITLC.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed]

Using human glioblastoma U87MG cells, the 50% inhibitory concentration of cMBP was determined to be 1.5 μM (6). In a blocking study, the cells were exposed to ^125^I-cMBP (2 pmol) in the presence of excess unlabeled cMBP (1 nmol), and a significant (P = 0.049) reduction in cellular binding of the radiochemical was observed compared with controls (6). Also, a scrambled peptide, containing amino acids similar to the cMBP, had no effect on the binding of ^125^I-cMBP to the cells. Almost no ^125^I-cMBP was internalized by the cells as determined with cell internalization studies (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+rodentia)]

The biodistribution of ^125^I-cMBP was studied in mice (n = 5 animals/time point) bearing U87MG cell xenograft tumors (6). The animals were injected with the radiochemical through the tail vein and euthanized at predetermined time points from 30 min to 24 h after the treatment. Tissues and organs of interest were subsequently removed from the animals; accumulated radioactivity was measured with a gamma counter, and the accumulated radioactivity data was presented as percent of injected dose per gram tissue (% ID/g). A high uptake of radioactivity by the pancreas was reported (47.28 ± 4.39% ID/g at 30 min, 58.37 ± 26.05% ID/g at 6 h, and 1.15 ± 1.89% ID/g at 24 h). The tumor uptake was 9.3 ± 0.78% ID/g at 30 min and decreased to 0.19 ± 0.31% ID/g by 24 h. A high uptake of the label by the kidneys was also observed (17.18 ± 1.12% ID/g at 30 min, 7.32 ± 3.17% ID/g at 6 h, and 0.29 ± 0.40% ID/g at 24 h). All other organs showed a similar distribution of radioactivity at the different time points (for details, please see Table 1 of Kim and Park, et al. (6)). The tumor/blood ratio was reported to be 1.89 at 4 h after treatment with the radiolabel. Because of the high uptake of ^125^I-cMBP by the pancreas, the expression of c-Met in this organ was investigated using the reverse-transcriptase polymerase chain reaction. A low expression of c-Met was observed in the pancreas, indicating that the uptake of ^125^I-cMBP by this organ was not c-Met–mediated, and accumulation of label in this organ was non-specific. No blocking studies were reported.

From these studies, the investigators concluded that although ^125^I-cMBP was taken up by c-Met–expressing tumors, it was not a suitable imaging agent because it generated a high background due to accumulation in other tissue and organs of the animals (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cMBP-GGG-Cy5.5+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

No information is currently available.

## References

1 Naran S., Zhang X., Hughes S.J. (2009). Inhibition of HGF/MET as therapy for malignancy. Expert Opin Ther Targets.
2 Abounader R., Laterra J. (2005). Scatter factor/hepatocyte growth factor in brain tumor growth and angiogenesis. Neuro Oncol.
3 Birchmeier C., Birchmeier W., Gherardi E., Vande Woude G.F. (2003). Met, metastasis, motility and more. Nat Rev Mol Cell Biol.
4 Kim E.M., Park E.H., Cheong S.J., Lee C.M., Jeong H.J., Kim D.W., Lim S.T., Sohn M.H. (2009). In vivo imaging of mesenchymal-epithelial transition factor (c-Met) expression using an optical imaging system. Bioconjug Chem.
5 Kim K., Hur Y., Ryu E.K., Rhim J.H., Choi C.Y., Baek C.M., Lee J.H., Chung J. (2007). A neutralizable epitope is induced on HGF upon its interaction with its receptor cMet. Biochem Biophys Res Commun.
6 Kim E.M., Park E.H., Cheong S.J., Lee C.M., Kim D.W., Jeong H.J., Lim S.T., Sohn M.H., Kim K., Chung J. (2009). Characterization, biodistribution and small-animal SPECT of I-125-labeled c-Met binding peptide in mice bearing c-Met receptor tyrosine kinase-positive tumor xenografts. Nucl Med Biol.
7 Chopra, A., 125I labeled mesenchymal-epithelial transition factor binding peptide-Gly-Gly-Gly. [125I-cMBP-GGG]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
8 Chopra, A., 125I labeled mesenchymal-epithelial transition factor binding peptide-8-aminooctanoic acid linker. [125I-cMBP-AOC]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Chopra, A., Mesenchymal-epithelial transition factor binding peptide-Gly-Gly-Gly-conjugated to Cy5.5 [cMBP-GGG-Cy5.5]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
10 Chopra, A., Mesenchymal-epithelial transition factor binding peptide with an 8-aminooctanoic acid linker conjugated to Cy5.5. [cMBP-AOC-Cy5.5]. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.